# [^99m^Tc]-Acetyl-arg-arg-arg-arg-arg-cys-gly-cys-gly-gly-pro-leu-tyr-arg-arg-ile-ile-arg-arg-leu-leu-glu-ser-dermatan sulfate

Chemical name: | [^99m^Tc]-Acetyl-arg-arg-arg-arg-arg-cys-gly-cys-gly-gly-pro-leu-tyr-arg-arg-ile-ile-arg-arg-leu-leu-glu-ser-dermatan sulfate
Abbreviated name: | ^99m^Tc-P1827DS
Synonym:
Agent Category: | Compound
Target: | Leukocytes (binding site unknown)
Target Category: | Unknown binding site
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Non-human primates

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P1827)]

The characteristic ability of white blood cells (WBC) to accumulate at sites of infection and inflammation has been used as a tool for the detection of these pathological conditions. The leukocyte and monocyte components of the WBC have often been labeled under ex vivo conditions with radionuclides such as indium (^111^In), meta-stable technetium (^99m^Tc), or radioactive compounds such as ^99m^Tc-gluceptate, [^67^Ga]gallium citrate, and ^99m^Tc-labeled antibodies, for the detection of infection or inflammation (1). Radiolabeling of leukocytes or monocytes involves the isolation of these cells from the WBC pool, a process that is slow and expensive, requires the handling of possibly infectious blood, and can lead to contamination of the samples. In addition, the labeled cells have a slow clearance from circulation and may be imaged up to 24 h after administration to allow time for accumulation at the site of infection or inflammation. Also, the labeled cells usually have a low signal-to-noise ratio, especially during the early time points, and show a high intestinal uptake that interferes with diagnostic imaging of the abdominal area (2).

Monoclonal antibodies labeled with radioactivity have also been used to image infections, but these radiopharmaceuticals have limited application because they also had a slow clearance from circulation and are not always sensitive enough to detect pulmonary or bone infections (3, 4). In addition, labeled antibodies have been shown to induce transient neutropenia and the formation of human anti-mouse antibodies (HAMA) in patients (4, 5). Therefore, repeat use of the antibodies can be limited by the HAMA response because it neutralizes and alters the biodistribution of the agent (6). The use of peptides to detect infection or inflammation is an attractive option because these compounds are cheap and easy to synthesize, can be modified to suit target requirements, and show rapid clearance from circulation (7, 8). Chemotactic peptides have been developed and evaluated for the imaging of infections and inflammation, but these compounds have limitations because the buffer components used to label the peptides may influence their biodistribution characteristics (8). Moyer et al. identified and developed a heparin-binding peptide, P483, for the imaging of infections (9). The sequence of this peptide was based on the platelet factor-4 heparin-binding region and was modified to contain a lysine-rich region to allow rapid renal clearance. It also contains a cys-gly-cys sequence to facilitate the formation of a coordination complex with ^99m^Tc. The peptide was complexed with heparin to enhance binding to WBC and labeled with ^99m^Tc to generate a labeled peptide (^99m^Tc-P483H) that was shown to target leukocytes (9). The labeled peptide was evaluated for the imaging of infections in a rabbit model as well as in humans (9, 10). Although ^99m^Tc-P483H was safe and could detect infections rapidly and accurately, it showed accumulation in the thyroid, salivary gland, and gastrointestinal tract (10).

In an effort to develop an improved imaging agent for infections compared to P483H, Krause et al. synthesized a peptide with a modified amino acid sequence (11). They substituted all the lysine residues of P483 with arginine to obtain Ac-arg-arg-arg-arg-arg-cys-gly-cys-gly-gly-pro-leu-tyr-arg-arg-ile-ile-arg-arg-leu-leu-glu-ser (P1827). This molecule was subsequently complexed with radioactive technetium (^99m^Tc) and dermatan sulfate (DS), a more homogeneous molecule compared to heparin, to obtain ^99m^Tc-P1827DS. The labeled peptide was then evaluated for the detection of infection in a rabbit model and compared to ^99m^Tc-labeled interleukin 8 (IL-8), which has been shown to successfully detect infection and inflammation in a variety of models (12-15). Results obtained with ^99m^Tc-P1827DS were also compared to those obtained with ^99m^Tc-P483H (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^99m^Tc-P1827DS was performed with commercially available amino acids with the use of solid-phase technology on a peptide synthesizer with N-α-Fmoc protection as described by some investigators (11, 16). The peptide was then purified with preparative reverse-phase high-performance liquid chromatography (RP-HPLC) and lyophilized as a trifluoroacetate (TFA) salt. Purity and composition of the peptide was confirmed with RP-HPLC and fast atom bombardment or electrospray mass spectrometry.

A lyophilized kit containing 0.05 μM P1827, tin chloride dehydrate, sodium glucoheptonate dihydride, and sodium ethylenediamine tetraacetic acid was reconstituted with ^99m^Tc-labeled sodium pertechnetate and heated in a boiling water bath for 10 min. The vial was cooled and 0.005 μM DS was added to it. This ratio of labeled peptide to DS was determined to be optimal for maximum accumulation of the label at the site of infection (11). Radiochemical purity (RCP) of the preparations was analyzed with thin-layer chromatography on Gelman saturator pad strips with isopropyl alcohol and water as one of the developing solvents. Under these conditions the R_f_ of ^99m^Tc-pertechnetate, ^99m^Tc-P1827, and ^99m^Tc-hydrophobic species was >0.75. When sodium dodecyl sulfate and water (SDS:W) was used as the developing agent, the R_f_ was <0.75.for the ^99m^Tc-radiocolloids. The RCP was calculated as 100% – (% radioactivity at R_f_ > 0.75 + % radioactivity at R_f_ <0.75). The RCP for all preparations used for the study was >90% (11). Specific activity of the labeled peptide used for the various studies was reported to be 14 μCi/40 pmol (518 kBq/40pmol). The investigators reported that, although ^99m^Tc-P1827 and DS solutions were clear, mixture of the two components produced a turbid solution. On centrifugation of the turbid solution, 95% of the activity was found in the pellet. However, when ^99m^Tc-P1827DS was mixed with 10 volumes of human or rabbit plasma and incubated for 30 min at 37°C, 33–37% of the radioactivity was found in the supernatant after centrifugation.

The synthesis of ^99m^Tc-labeled P483H and hydrazinonicotinamide (HYNIC)-conjugated IL-8, used for the comparison of results obtained with ^99m^Tc-P1827DS, was described in detail by Krause et al. (11). A comparison with HYNIC–IL-8 was made because it has previously been evaluated for the detection of infection and inflammation under various experimental conditions (11). The specific activity and RPC of these labeled compounds were not provided in the publication.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P1827DS+in+vitro&WebEnv=072phqj8bYhxreGm5uEtq_kOh8LqKWDaEmOT0vP-AzT8uduPDupZZnxgQKoVl8GFCJHbZu_9aERGlHD%407748428072881B60_0000SID&WebEnvRq=1)]

The in vitro binding of ^99m^Tc-P1827DS was studied in human blood cells (11). The labeled peptide was incubated with whole human blood for 2 h at 37°C and layered on a gradient cushion to separate the various cell populations by centrifugation. Each fraction was isolated, washed twice with buffer, and counted for bound radioactivity. The labeled peptide was found to bind primarily to the leukocytes and not to the erythrocytes. Binding to the leukocytes was not saturable even at a maximum concentration of 10 μM used in the study. Activation of leukocytes with lipopolysaccharide was observed to increase the binding of the labeled peptide to the cells.

### Animal Studies

### Rodents

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P1827DS+Non-Primate+Mammals&WebEnv=05GT2e_s_9_7lFtGIPViV4QI0BZ-HqtEiZES4WJEDA0egpRG_wZvg4r0Id_U8zA_8DWhsEA2EuxIJGb%407748428072881B60_0000SID&WebEnvRq=1)]

Accumulation of the labeled peptide at an infection site was studied in rabbits injected with Escherichia coli in the right calf muscle (11). The infected animals (n = 6 per group) were injected with ^99m^Tc-P1827DS or, for comparison, with ^99m^Tc-P483H in the marginal ear vein and euthanized 4 h after administration of the labeled compounds. The various tissues were removed and weighed, and the incorporated radioactivity was determined. Scintigraphic images of the animals were acquired 4 h after injection of the radioactivity. Both agents were reported to have accumulated at the infection site (11). However, between the two agents, ^99m^Tc-P1827DS had a higher infected muscle/blood ratio (28.2 ± 12.1 compared to that of 9.5 ± 4.5 for ^99m^Tc-P483H). Both agents showed an accumulation in the lungs and the spleen. The accumulation of ^99m^Tc-P1827DS was lower in the gastrointestinal tract, thyroid, and palate, indicating that this agent had a superior stability of the Tc chelate compared to its predecessor, ^99m^Tc-P483H.

The uptake and biodistribution of ^99m^Tc-P1827DS at the infected site were also compared to those of ^99m^Tc-HYNIC–IL-8in rabbits infected with E. coli (n = 5 animals per group) as described above (11). The abscesses were visible by scintigraphy with both agents 1 h after administration of the label, and the sites were clearly delineated at 4 h. A higher accumulation of ^99m^Tc-HYNIC–IL-8, compared to ^99m^Tc-P1827DS, was evident at 6 h. The infected muscle/blood ratios for the two agents were 48.2 ± 21.3 and 26.7 ± 8.4, respectively. A very high accumulation of ^99m^Tc-HYNIC–IL-8 was observed in the kidneys, but a high amount of ^99m^Tc-P1827DS accumulated in the lungs. A slightly higher amount of ^99m^Tc-P1827DS, compared to ^99m^Tc-HYNIC–IL-8, accumulated in the liver and spleen (11). With results obtained from these studies, the investigators concluded that ^99m^Tc-P1827DS was not a superior infection imaging agent compared to ^99m^Tc-HYNIC–IL-8 (11).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P1827DS+Non+Human+Primates&WebEnv=0KA5QA6SKeqwT1hN2tbrt8O3-e8UO0gRDut97nWfRlsmKN-oOpgCjIWQqOajfcwMKCwCs-u9ZUEQqN_%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P1827DS+Humans&WebEnv=0MpZhnHD9r0MWmdg6EyT62yrs06xLTMtS64i0jrhrdXwWe81eiBF7t5IoGTz99DRSIczQGJhOKUN_-N%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## References

1 Boerman O.C., Rennen H., Oyen W.J., Corstens F.H. (2001). Radiopharmaceuticals to image infection and inflammation. Semin Nucl Med.
2 Ballinger J.R., Gnanasegaran G. (2005). Radiolabelled leukocytes for imaging inflammation: how radiochemistry affects clinical use. Q J Nucl Med Mol Imaging.
3 Rubin R.H., Fischman A.J. (1994). The use of radiolabeled nonspecific immunoglobulin in the detection of focal inflammation. Semin Nucl Med.
4 Becker W., Bair J., Behr T., Repp R., Streckenbach H., Beck H., Gramatzki M., Winship M.J., Goldenberg D.M., Wolf F. (1994). Detection of soft-tissue infections and osteomyelitis using a technetium-99m-labeled anti-granulocyte monoclonal antibody fragment. J Nucl Med.
5 Thakur M.L., Li J., Chandy B., John E.K., Gibbons G. (1996). Transient neutropenia: neutrophil distribution and replacement. J Nucl Med.
6 Sakahara H., Reynolds J.C., Carrasquillo J.A., Lora M.E., Maloney P.J., Lotze M.T., Larson S.M., Neumann R.D. (1989). In vitro complex formation and biodistribution of mouse antitumor monoclonal antibody in cancer patients. J Nucl Med.
7 Fischman A.J., Babich J.W., Rubin R.H. (1994). Infection imaging with technetium-99m-labeled chemotactic peptide analogs. Semin Nucl Med.
8 Lister-James J., Moyer B.R., Dean T. (1996). Small peptides radiolabeled with 99mTc. Q J Nucl Med.
9 Moyer B.R., Vallabhajosula S., Lister-James J., Bush L.R., Cyr J.E., Snow D.A., Bastidas D., Lipszyc H., Dean R.T. (1996). Technetium-99m-white blood cell-specific imaging agent developed from platelet factor 4 to detect infection. J Nucl Med.
10 Palestro C.J., Weiland F.L., Seabold J.E., Valdivia S., Tomas M.B., Moyer B.R., Baran Y.M., Lister-James J., Dean R.T. (2001). Localizing infection with a technetium-99m-labeled peptide: initial results. Nucl Med Commun.
11 Krause S., Rennen H.J., Boerman O.C., Baumann S., Cyr J.E., Manchanda R., Lister-James J., Corstens F.C., Dinkelborg L.M. (2007). Preclinical evaluation of technetium 99m-labeled P1827DS for infection imaging and comparison with technetium 99m IL-8. Nucl Med Biol.
12 Gratz S., Rennen H.J., Boerman O.C., Oyen W.J., Burma P., Corstens F.H. (2001). (99m)Tc-interleukin-8 for imaging acute osteomyelitis. J Nucl Med.
13 Gratz S., Rennen H.J., Boerman O.C., Oyen W.J., Corstens F.H. (2001). Rapid imaging of experimental colitis with (99m)Tc-interleukin-8 in rabbits. J Nucl Med.
14 Rennen H.J., Boerman O.C., Oyen W.J., Corstens F.H. (2003). Kinetics of 99mTc-labeled interleukin-8 in experimental inflammation and infection. J Nucl Med.
15 Rennen H.J., Bleeker-Rovers C.P., van Eerd J.E., Frielink C., Oyen W.J., Corstens F.H., Boerman O.C. (2004). 99mTc-labeled interleukin-8 for scintigraphic detection of pulmonary infections. Chest.
16 Merrifield R.B. (1963). Solid-phase synthesis of peptides. Journal of American Chemical Society.